# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-Lys(Cy5.5)-Gly-Gly-Tyr-knottin 2.5D

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-Lys(Cy5.5)-Gly-Gly-Tyr-knottin 2.5D
Abbreviated name: | ^64^Cu-DOTA/Cy5.5-2.5D
Synonym:
Agent Category: | Peptide
Target: | α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors
Target Category: | Receptor
Method of detection: | Multimodality imaging: positron emission tomography (PET); optical, near-infrared (NIR) fluorescence
Source of signal / contrast: | ^64^Cu, Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=knottin+peptides)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled ligands have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ integrin (expressed as 50% inhibitory concentration (IC_50_), 7–40 nM) but not to α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM) integrins. Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Only one cyclic RGD peptide used for imaging, [^18^F]fluoropropionyl-galacto-c(Arg-Gly-Asp-D-Phe-Lys) ([^18^F]-galacto-RGD), has been investigated for measuring expression of the α_v_β_3_ integrin in cancer patients with tumors. However, [^18^F]-galacto-RGD has been shown to have low tumor accumulation and low signal/background ratios in humans. Cystine knot peptides (knottins) share a common disulfide-bonded framework and a triple-stranded β-sheet fold (13). The integrin-binding RGD motif was grafted into a knottin from the trypsin inhibitor II of the squirting cucumber plant (Ecballium elaterium). Knottin 2.5D (with three disulfide bonds (GCPQGRGDWAPTSCSQDSDCLAGCVCGPNGFCG-NH_2_)) was identified from a series of genetically engineered knottin peptides to exhibit nanomolar binding to the α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors (14, 15). Cy5.5 and ^64^Cu-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (^64^Cu-DOTA), were both chemically conjugated to the knottin N-terminus using a peptide-based linker, Lys-Gly-Gly-Tyr (16). The resulting agent, ^64^Cu-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Lys(Cy5.5)-Gly-Gly-Tyr-knottin 2.5D (^64^Cu-DOTA/Cy5.5-2.5D), has been evaluated for positron emission tomography (PET) and optical imaging of tumor xenografts in mice.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Knottin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Knottin (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=841163)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=knot%20peptide)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+synthesis)]

Knottin 2.5D was prepared with solid-phase peptide synthesis (16). The linear peptide was folded in the presence of 2.5 mM reduced glutathione and 20% dimethyl sulfoxide in 0.1 M ammonium bicarbonate (pH 9). Knottin 2.5D was purified with high-performance liquid chromatography. Peptide purity and molecular mass were confirmed with MALDI-TOF mass spectroscopy and electrospray ionization mass spectrometry. Knottin 2.5D was conjugated with Fmoc-Lys(ivDde)-Gly-Gly-Tyr-NHS ester and after removal of Fmoc to form NH_2_-Lys(ivDde)-Gly-Gly-Tyr-2.5D. NH_2_-Lys(ivDde)-Gly-Gly-Tyr-2.5D was incubated with five-fold excess of DOTA-NHS ester and removal of the ivDde group to form DOTA-Lys(NH_2_)-Gly-Gly-Tyr-2.5D, which was reacted with Cy5.5-NHS ester to yield DOTA-Lys(Cy5.5)-Gly-Gly-Tyr-2.5D. To label with ^64^Cu, DOTA-Lys(Cy5.5)-Gly-Gly-Tyr-2.5D was incubated with ^64^CuCl_2_ in 0.1 N sodium acetate (pH 6.3) for 1 h at 42°C. ^64^Cu-DOTA/Cy5.5-2.5D was purified with column chromatography with a yield of >80%. The radiochemical purity and specific activity were >95% and ~18.5 GBq/µmol (0.5 Ci/µmol), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=knottin+2%2E5D+in+vitro+studies)]

To determine the relative integrin-binding affinities (expressed as IC_50_ values) of echistatin, 2.5D, Cy5.5-2.5D, DOTA-2.5D,and, DOTA/Cy5.5-2.5D, a competition binding assay was performed with ^125^I-echistatin using U87MG human glioblastoma cells (16). The IC_50_ values for echistatin, 2.5D, Cy5.5-2.5D, DOTA-2.5D, and DOTA/Cy5.5-2.5D were determined to be 4 ± 1, 19 ± 6, 5 ± 1, 9 ± 3, and 30 ± 7 nM, respectively. DOTA/Cy5.5-2.5D exhibited strong binding to α_v_β_3_ and α_v_β_5_ integrins, and moderate binding to the α_5_β_1_ integrin.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=knottin+2%2E5D+rodentia)]

Kimura et al. (16) performed ex vivo biodistribution studies of 3.7 MBq (100 μCi) ^64^Cu-DOTA/Cy5.5-2.5D (0.5 nmol) at 1, 4, and 24 h after intravenous injection in nude mice (n = 3/group) bearing U87MG xenografts. Not a complete reference. Tracer accumulation values in the tumors at 1, 4, and 24 h were 3.24 ± 0.87%, 5.64 ± 0.83%, and 4.57 ± 0.70% injected dose per gram (ID/g), respectively. The organ with the highest accumulation of radioactivity at 4 h after injection was the kidney (~80% ID/g), followed by the liver (7% ID/g), lung (2% ID/g), and spleen (2% ID/g). The radioactivity in the blood was <0.5% ID/g. ^64^Cu-DOTA/Cy5.5-2.5D was ~80% intact in the blood at 1 h after injection, whereas the agent was ~60% intact in the tumor and <20% intact in the liver and kidney at the same time point. NIR fluorescent images of the organs and tumor tissue from mice injected with ^64^Cu-DOTA/Cy5.5-2.5D (0.5 nmol) were obtained at 1, 4, and 24 h after injection. The NIR flux/g in the tumors was 373, 360, and 146 at these time points, respectively. The organ with the highest NIR flux at 4 h after injection was the kidney (~2,000 flux/g), followed by the liver (100 flux/g), lung (60 flux/g), and spleen (50 flux/g). The radioactivity in the blood was <10 flux/g. Investigators reported good correlation (R^2^, 0.75–0.83) of tumor/tissue ratios for Cy5.5 and ^64^Cu accumulation at these time points.

PET analysis was performed after intravenous injection of 3.7 MBq (100 μCi) ^64^Cu-DOTA/Cy5.5-2.5D (0.5 nmol) in nude mice (n = 3) bearing U-87MG tumors. Tumors were clearly visualized at 1–2 h along with the kidneys, liver, and urinary bladder. Tumor accumulation was determined to be 4.27%, 4.19%, 4.52%, and 5.02% ID/g at 1, 2, 4, and 24 h after injection, respectively. Co-administration of 500 nmol c(RGDyK) decreased tumor accumulation to 1%–1.5% ID/g at 1–24 h after injection (P < 0.05). NIR fluorescence imaging with DOTA/Cy5.5-2.5D (1.5 nmol) in nude mice (n = 3) bearing U-87MG xenografts. The tumor/background ratios were 2.96, 3.11, 3.60, and 4.04 at 1, 2, 4, and 24 h after injection, respectively. Co-administration of 500 nmol c(RGDyK) decreased tumor accumulation to 2.47 at 24 h after injection (P < 0.05).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=knottin%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=knottin+2%2E5D+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=knottin+2%2E5D+Human+Studies)]

No references are currently available.

## NIH Support

5K01 CA104706, P50 CA114747, R25 CA118681

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Pallaghy P.K., Nielsen K.J., Craik D.J., Norton R.S. (1994). A common structural motif incorporating a cystine knot and a triple-stranded beta-sheet in toxic and inhibitory polypeptides. Protein Sci.
14 Kimura R.H., Levin A.M., Cochran F.V., Cochran J.R. (2009). Engineered cystine knot peptides that bind alphavbeta3, alphavbeta5, and alpha5beta1 integrins with low-nanomolar affinity. Proteins.
15 Kimura R.H., Cheng Z., Gambhir S.S., Cochran J.R. (2009). Engineered knottin peptides: a new class of agents for imaging integrin expression in living subjects. Cancer Res.
16 Kimura, R.H., Z. Miao, Z. Cheng, S.S. Gambhir, and J.R. Cochran, A Dual-Labeled Knottin Peptide for PET and Near-Infrared Fluorescence Imaging of Integrin Expression in Living Subjects. Bioconjug Chem, 2010